# Quantum dot 800–mercaptopropionic acid

Chemical name: | Quantum dot 800–mercaptopropionic acid
Abbreviated name: | QD800-MPA
Synonym:
Agent category: | Compound
Target: | Non-targeted
Target category: | Non-targeted
Method of detection: | Optical, near-infrared fluorescence (NIR)
Source of signal: | Quantum dot (QD)
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=QD800)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a noninvasive alternative to radionuclide imaging in small animals (4).

Fluorescent semiconductor quantum dots (QDs) are nanocrystals made of CdSe/CdTe/ZnS with radii of 1–10 nm (5-7). They can be tuned to emit fluorescence signals in a range of wavelengths by changing their sizes and composition, thus providing broad excitation profiles and high absorption coefficients. They have narrow, symmetric emission spectra with long, excited-state lifetimes (20–50 ns) compared with those of fluorescent dyes (1–10 ns). They process good quantum yields of 40%–90% and possess high extinction coefficients. They are more photo-stable than conventional organic dyes. They can be coated and capped with hydrophilic materials for additional conjugation with biomolecules, such as peptides, antibodies, nucleic acids, and small organic compounds, which have been tested in vitro and in vivo (7-11). Although many cells have been labeled with QDs in vitro with little cytotoxicity, there are limited studies of long-term toxicity of QDs in small animals (12-20); little is known about the toxicity and the mechanisms of clearance and metabolism of QDs in humans.

QDs that do not contain Cd (non-Cd QDs) have been prepared as an alternative to the more toxic Cd-based QDs. These newly developed non-Cd QDs exhibit improved blood half-life and minimal reticuloendothelial system (RES) accumulation with rapid renal clearance (21). These QDs easily extravasate leaky tumor blood vessels because of the enhanced permeability and retention effect. Mercaptopropionic acid (MPA)-coated InAs/InP/ZnSe QDs (QD800-MPA) have been evaluated for NIR fluorescence imaging tumor in mice (21, 22).

### Related Resource Links:

- Chapters in MICAD (QDs (http://www.ncbi.nlm.nih.gov/books?term=Quantum%20dot%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=QD800%20MPA%20and%20synthesis)]

Non-Cd QDs (InAs/InP/ZnSe) (QD800, 1 nmol In) with an emission maximum at 800 nm was mixed with 5 mM MPA (pH 8) in chloroform for 4 h. QD800-MPA was isolated with centrifugation to remove excess MPA (22). QD800-MPA had a hydrodynamic diameter of 8.2 nm. QD800 ITK carboxyl (QD800-COOH) was purchased from Invitrogen as a control; it is composed of Cd/Te/ZnS and has a hydrodynamic diameter of 25 nm. QD800-MPA-HSA was prepared by mixing 1,000 nmol QD800-MPA with 15 nmol human serum albumin (HSA). QD800-MPA-HSA had a hydrodynamic diameter of 18 nm.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=QD800%20MPA%20and%20in%20vitro)]

Xie et al. (21) showed that QD800-MPA (10 nM, In) was less toxic than QD800-COOH (10 nM) to RAW 264.7 mouse macrophage cells after incubation for 24 h at 37°C. QD800-MPA exhibited 10% cytotoxicity, whereas QD800-COOH showed 50% cytotoxicity. Cell cytotoxicity for QD800-MPA and QD800-COOH increased to 50% and 65% at 48 h, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=QD800%20MPA%20and%20rodentia)]

Gao et al. (22) performed tumor-imaging studies with QD800-MPA in nude mice (n = 3/group) bearing 22B or LS174T tumors. Whole-body small animal images were obtained with reflectance planar fluorescence after intravenous injection of QD800-MPA (0.2 nmol), QD800-COOH (0.2 nmol), or QD800-MPA-HSA (0.1 nmol). Intense tumor signals were obtained in both tumors (passive targeting by enhanced vascular permeability) at 1 h after injection of QD800-MPA with low signal intensity from other organs. Tumor intensity increased over time with good fluorescence contrast at 4 h. Ex vivo biodistribution was studied at 4 h with mice bearing 22B tumors. Tumor accumulation was 11.0 ± 2.0% injected dose/gram (ID/g). The tissue with the highest accumulation was the liver (42.6 ± 6.4% ID/g), followed by the kidney (18.9 ± 1.9% ID/g), spleen (10.2 ± 2.9% ID/g), and lung (3.2 ± 1.4% ID/g). The tumor/background ratios were ~4 at 0.5, 1, and 4 h and decreased to 1.1 at 24 h. The biodistribution pattern obtained with region of interest fluorescence analysis was similar. Histological analysis of tumor sections showed that QD800-MPA was present in the interstitial space and tumor vessels. On the other hand, QD800-COOH showed tumor/background ratios of ~1 from 0.5 h to 24 h after injection. QD800-COOH showed one-fold higher accumulation in the liver and four-fold lower accumulation in the kidney than QD800-MPA at 4 h after injection. Tumor accumulation of QD800-MPA-HSA at 4 h after injection was 23.0 ± 2.4% ID/g; liver accumulation was 27.0% ID/g at 4 h after injection, and spleen accumulation was 5% ID/g at the same time point. QD800-MPA-HSA was considered to be more suitable than QD800-MPA as an imaging agent because it exhibited lower RES accumulation and higher tumor accumulation. QD800-MPA-HSA and QD-MPA were eliminated mainly by renal clearance. Xie et al. (21) determined that the circulation half-life of QD800-MPA in normal nude mice was 110 min, whereas the half-life for QD800-COOH was only 6 min.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=QD800%20MPA%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=QD800%20MPA%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=QD800%20MPA%20and%20human%20not%20animal%20not%20cell%20line)]

No publication is currently available.

## NIH Support

R21 CA121842, P50 CA114747, U54 CA119367, R21 CA121842

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
3 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
4 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
5 Chan W.C., Maxwell D.J., Gao X., Bailey R.E., Han M., Nie S. (2002). Luminescent quantum dots for multiplexed biological detection and imaging. Curr Opin Biotechnol.
6 Gao X., Nie S. (2005). Quantum dot-encoded beads. Methods Mol Biol.
7 Michalet X., Pinaud F.F., Bentolila L.A., Tsay J.M., Doose S., Li J.J., Sundaresan G., Wu A.M., Gambhir S.S., Weiss S. (2005). Quantum dots for live cells, in vivo imaging, and diagnostics. Science.
8 Alivisatos A.P., Gu W., Larabell C. (2005). Quantum dots as cellular probes. Annu Rev Biomed Eng.
9 Hilger I., Leistner Y., Berndt A., Fritsche C., Haas K.M., Kosmehl H., Kaiser W.A. (2004). Near-infrared fluorescence imaging of HER-2 protein over-expression in tumour cells. Eur Radiol.
10 Medintz I.L., Uyeda H.T., Goldman E.R., Mattoussi H. (2005). Quantum dot bioconjugates for imaging, labelling and sensing. Nat Mater.
11 Smith A.M., Gao X., Nie S. (2004). Quantum dot nanocrystals for in vivo molecular and cellular imaging. Photochem Photobiol.
12 Akerman M.E., Chan W.C., Laakkonen P., Bhatia S.N., Ruoslahti E. (2002). Nanocrystal targeting in vivo. Proc Natl Acad Sci U S A.
13 Braydich-Stolle L., Hussain S., Schlager J.J., Hofmann M.C. (2005). In vitro cytotoxicity of nanoparticles in mammalian germline stem cells. Toxicol Sci.
14 Frangioni J.V., Hajjar R.J. (2004). In vivo tracking of stem cells for clinical trials in cardiovascular disease. Circulation.
15 Gao X., Cui Y., Levenson R.M., Chung L.W., Nie S. (2004). In vivo cancer targeting and imaging with semiconductor quantum dots. Nat Biotechnol.
16 Han M., Gao X., Su J.Z., Nie S. (2001). Quantum-dot-tagged microbeads for multiplexed optical coding of biomolecules. Nat Biotechnol.
17 Lovric J., Bazzi H.S., Cuie Y., Fortin G.R., Winnik F.M., Maysinger D. (2005). Differences in subcellular distribution and toxicity of green and red emitting CdTe quantum dots. J Mol Med.
18 Ohnishi S., Lomnes S.J., Laurence R.G., Gogbashian A., Mariani G., Frangioni J.V. (2005). Organic alternatives to quantum dots for intraoperative near-infrared fluorescent sentinel lymph node mapping. Mol Imaging.
19 Shiohara A., Hoshino A., Hanaki K., Suzuki K., Yamamoto K. (2004). On the cyto-toxicity caused by quantum dots. Microbiol Immunol.
20 Soltesz E.G., Kim S., Laurence R.G., DeGrand A.M., Parungo C.P., Dor D.M., Cohn L.H., Bawendi M.G., Frangioni J.V., Mihaljevic T. (2005). Intraoperative sentinel lymph node mapping of the lung using near-infrared fluorescent quantum dots. Ann Thorac Surg.
21 Xie R., Chen K., Chen X., Peng X. (2008). InAs/InP/ZnSe Core/Shell/Shell Quantum Dots as Near-Infrared Emitters: Bright, Narrow-Band, Non-Cadmium Containing, and Biocompatible. Nano Res.
22 Gao J., Chen K., Xie R., Xie J., Lee S., Cheng Z., Peng X., Chen X. (2010). Ultrasmall near-infrared non-cadmium quantum dots for in vivo tumor imaging. Small.